# ^64^Cu-Labeled 1,1’-{1,4-phenylenebis(methylene)}-bis{1,4,8,11-tetraaza-cyclotetradecane}

Chemical name: | ^64^Cu-Labeled 1,1’-{1,4-phenylenebis(methylene)}-bis{1,4,8,11-tetraaza-cyclotetradecane}
Abbreviated name: | [^64^Cu]-AMD3100
Synonym: | [^64^Cu]-4
Agent Category: | Ligand
Target: | Chemokine receptor 4 (CXCR4)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of AMD3100 for additional information regarding the compound in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

The chemokine receptor 4 (CXCR4) and its ligand, the stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and the hematopoietic systems (1, 2). In addition, this receptor–ligand pair has a function in the development, progression, and spread of various cancers (3), and the CXCR4 acts as a co-receptor to facilitate entry of the human immunodeficiency virus (HIV) into CD4^+^ cells (4). It has also been suggested that CXCR4 and SDF-1 participate in the pathogenesis of neurodegenerative and inflammatory conditions (5). Because of its role in the development of cancer and HIV infections, a variety of CXCR4 inhibitors, including 1,1’-{1,4-phenylenebis(methylene)}-bis{1,4,8,11-tetraaza-cyclotetradecane} (AMD3100), have been evaluated for the treatment of these ailments (6, 7).

Some imaging studies have also been performed on CXCR4 (8, 9). Technetium (^99m^Tc)-labeled SDF-1 was shown to be a suitable probe to quantify CXCR4 levels under in vivo conditions and could be used to determine changes in CXCR4 expression in different tissue under various pathological and physiological conditions (8). An indium (^111^In)-labeled CXCR4 antagonist, [^111^In]-Ac-TZ14011, was developed for the imaging of CXCR4 expression in xenograft tumors in mice, and Hanaoka et al. used single-photon emission computed tomography to investigate the biodistribution of [^111^In]-Ac-TZ14011 in mice (9). However, the labeled compound showed a low accumulation in the tumors (<1% of the injected dose/gram tissue (% ID/g)), and a high accumulation was reported in the liver (19.3% ID/g), kidneys (29.5% ID/g), and the spleen (5.83% ID/g). These results indicated that [^111^In]-Ac-TZ14011 was suitable for the imaging of CXCR4, although it lacked tumor specificity and the high accumulation of radioactivity in the liver and kidneys showed that this radiochemical was not suitable for the imaging of tumors in these organs.

In an effort to develop a superior CXCR4 imaging agent, AMD3100 was labeled with radioactive copper (^64^Cu) to produce [^64^Cu]-AMD3100, and it was evaluated as a positron emission tomography imaging agent by Jacobson et al. (10). The investigators also studied the biodistribution of [^64^Cu]-AMD3100 in normal mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+synthesis)]

The synthesis of AMD3100 was described by Jacobson et al. (10). AMD3100 was labeled with ^64^Cu by the addition of ^64^Cu-acetate to a solution of AMD3100 dissolved in 0.4 M ammonium acetate (pH 5.5) followed by stirring for 1 h at room temperature (10). Radiochemical purity of [^64^Cu]-AMD3100 was determined with thin-layer chromatography (TLC). The Rf of labeled AMD3100 was reported to be ~0.1, and that of free ^64^Cu was ~0.6, as determined with TLC. Although the radiochemical labeling yield was not stated the radiochemical yield and purity of [^64^Cu]-AMD3100 were reported to be 100%, respectively, under these analytical conditions. The radiotracer had a specific activity of 417 TBq/mmol (11,280 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+in+vitro)]

Using a cell binding assay the 50% inhibitory concentration (IC_50_) of [^64^Cu]-AMD3100 for Jurkat cells (which were shown to have a high expression of the CXCR4 (10)) was reported to be 62.7 μM (10). A similar study by the investigators showed that the IC_50_ of [^64^Cu]-AMD3100 for mouse splenocytes was 46.9 μM.

To confirm that no changes had occurred in the biological activity (CXCR4 inhibition potential) of Cu-AMD3100, due to the incorporation of Cu, the ability of Cu-AMD3100 to inhibit Jurkat cell migration toward stromal cell-derived factor-1 in a transwell migration assay was compared to that of AMD3100 under the same experimental conditions (10). The IC_50_s of AMD3100 and Cu-AMD3100 required to inhibit the Jurkat cell migration were reported to be 27.4 and 75.4 nM, respectively.

The exact reasons for the discrepancy observed between the IC_50_ values reported for the binding and the transwell migration assays were not provided by the investigators.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+rodentia)]

Jacobson et al. studied the biodistribution of [^64^Cu]-AMD3100 in six groups of normal C57BL/6 mice (n = 5 animals/group) (10). Three groups of animals received intravenous injections of [^64^Cu]-AMD3100 and were euthanized 1, 2, and 6 h later. Groups four and five were co-injected with [^64^Cu]-AMD3100 and excess (50 μg) unlabeled AMD3100. These animals were euthanized 2 and 6 h after injection. The sixth group was injected with [^64^Cu]-AMD3100 in the presence of SDF-1 to determine specificity of the radiopharmaceutical for binding to CXCR4. These animals were euthanized 2 h after treatment. The thymus, liver, spleen, intestine, femoral bone marrow, muscle, blood, kidneys, and lymph nodes were removed from all the animals to determine accumulation of radioactivity in the various organs of the groups treated with [^64^Cu]-AMD3100,. In animals treated with [^64^Cu]-AMD3100 alone, the maximum accumulation of radioactivity was observed in the liver (~40–55% ID/g at the different time points), followed by spleen and bone marrow (~12–15% ID/g at the various time points), lymph nodes (~10% ID/g at all the time points), and the kidneys (~7% ID/g at the predetermined time points). Animals co-injected with the radiopharmaceutical and the unlabeled AMD3100 showed a reduced accumulation of radioactivity in the liver, bone marrow, and the lymph nodes 6 h after injection, which indicated that the radioactivity bound specifically to the CXCR4 in these organs (for details, please see Figure 7 in Jacobson et al. (10)).

Imaging of animals (n = 5 mice) injected with [^64^Cu]-AMD3100 alone revealed that the label accumulated mainly in the liver, kidneys, and spleen as observed during the biodistribution studies described above (10). Blocking of [^64^Cu]-AMD3100 uptake with excess unlabeled AMD3100 (n = 5 mice) resulted in a reduced accumulation of radioactivity in these organs. During the same time, imaging showed an accumulation of radioactivity in the kidneys. To confirm that the accumulated radioactivity in the animals (n = 5 mice) was not due to free ^64^Cu, the mice were treated with the free ^64^Cu isotope and scanned 2 h later. In these animals the radioactivity accumulated mainly in the liver and intestines, but not in the spleen and lymph nodes, which are known to contain a high level of CXCR4 receptors. This indicated that free ^64^Cu accumulated primarily in organs involved in the excretion of the labeled metal and that the radioactivity observed in the spleen and the lymph nodes during the biodistribution and imaging studies was from the labeled AMD3100.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AMD3100+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## NIH Support

Intramural Research Programs of the National Institute of Biomedical Imaging and Bioengineering and the National Institute of Allergy and Infectious Diseases.

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Kuritzkes D.R. (2009). HIV-1 entry inhibitors: an overview. Curr Opin HIV AIDS.
7 Otsuka S., Bebb G. (2008). The CXCR4/SDF-1 chemokine receptor axis: a new target therapeutic for non-small cell lung cancer. J Thorac Oncol.
8 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
9 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
10 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.